# Perflutren lipid microspheres

Chemical name: | Perflutren-lipid microspheres
Abbreviated name: | DMP 115
Synonym: | Definity^®^ ; octafluoropropane-lipid microspheres; liposome-encapsulated perfluoropane microspheres, YM454, 1,1,1,2,2,3,3,3-octafluoropropane-lipid microspheres
Agent Category: | Lipid microspheres
Target: | Non-targeted, blood pool
Target Category: | Passive nonspecific filling of cardiac chambers
Method of detection: | Ultrasound (US)
Source of signal/ contrast: | Microbubble and perflutren gas
Activation: | No
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=definity%20OR%20%22perflutren%20lipid%20microsphere%22)]

Perflutren lipid microspheres (DMP 115) is a preparation of liposome-encapsulated microspheres containing perflutren that was developed as an ultrasound (US) contrast agent for use in echocardiography to enhance US images (1, 2). In the United States, it is approved by the Food and Drug Administration (FDA) for clinical use in patients with suboptimal echocardiograms to opacify the left ventricular chamber (LV) and to improve the delineation of the left ventricular endocardial border (3).

US contrast agents, or echopharmaceuticals, are designed to change the attenuation (absorption, reflection, and refraction) or impedance (resistance to sound propagation) of sound for enhancing the differentiation of the signal (echo) of a target organ from that of the surrounding tissue (4-7). Gas-liquid emulsions (microbubbles or gaseous particles) are highly echogenic invivo because of the nonlinear rarefaction and compression effects that lead to volume pulsations of microbubbles (5, 8, 9). Human serum albumin, synthetic polymers and phospholipids have been used to construct the membranes of these bubbles. Microbubble preparations of various formulations have been developed, and their clinical usefulness depends very much on the size and stability of these bubbles in vivo. The current clinical application of these agents is in myocardial contrast echocardiography (MCE) (10).

Perfluorocarbons (PFCs) are inert, volatile chemicals and can be encapsulated within microbubbles to provide a stabilizing effect. The extremely low water solubility of PFCs (from 0.19 mol/m^3^ for n-C_3_F_8_ to 2.7 х 10−^4^ mol/m^3^ for n-C_6_F_14_) sets up an equilibrium in vivo in the water-soluble gases diffuse in and out of the microbubble, but the PFC vapor counterbalances the surface tension and blood pressure forces that push the gases inside the bubble toward dissolution. As a result, the combined properties of the microbubble shell and the PFC gas inside determine the stability and output signal of each microbubble in vivo. PFC emulsions were initially studied as oxygen carriers (blood substitutes) (11, 12). Perfluorooctyl bromide (C_8_BrF_17_), a compound similar to perflutren (C_3_F_8_; octafluoropropane or 1,1,1,2,2,3,3,3-octafluoropropane), was first discovered to possess sufficient lipophilicity to be formulated into stable emulsions, but it was developed as an oral agent for negative magnetic resonance imaging of the gastrointestinal tract (13). Perflutren has a boiling point of −37 º C and can be encapsulated as PFC gas within microbubbles (14).

DMP 115 was developed based on the perfluorocarbon liquid/gas-phase shift-based system with perflutren gas encapsulated within lipid microspheres (3, 5). The lipid formulation is a blend of dipalmitoylphosphatidylcholine (DPPC), a methylpoly(ethylene glycol) dipalmitoylphosphatidylethanolamine (MPEG5000 DPPE) and a small amount of negatively charged dipalmitoylphosphatidic acid (DPPA). These components are stored refrigerated under a headspace of perflutren gas before use. The recommended dose for clinical use is 10 µl/kg of body weight by i.v. bolus injection (30-60 sec). A second 10 µl/kg dose may be administered 30 min after the first dose.

Serious cardiopulmonary reactions following the administration of ultrasound microbubble contrast agents have been reported (15). In 2007, the US FDA (http://www.fda.gov/cder/drug/InfoSheets/HCP/microbubbleHCP.htm) requested that warnings emphasizing the risk for serious cardiopulmonary reactions be added to the labeling of these agents. The uses of these agents are contraindicated in patients with unstable cardiopulmonary status.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Definity%20OR%20%22Perflutren%20Lipid%20Microsphere%22%20OR%20Perflutren%29%20AND%20synthesis)]

PFCs are inert organic materials initially developed for handling the extremely corrosive uranium fluorides (11, 12, 16). Some PFCs are derived directly from the manufacturing line that led to Teflon and other diverse industrial surfactants. Two major strategies are commonly used in producing PFCs. One strategy is substituting fluorine atoms for hydrogen atoms in the parent hydrocarbon analog by electrochemical fluorination, fluorination by high-valence metal fluorides, or direct fluorination. Another strategy is combining smaller, reactive fluorinated building blocks by telomerization. Perflutren can be produced by fluorination of hexafluoropropylene with cobalt trifluoride (14). Pashkevish et al. (14) also described the synthesis of perflutren by high-temperature reaction of graphite with fluorine in a fluidized bed.

Egg phosphatidylcholine and synthetic phospholipids have been used to produce the microbubbles in the emulsion preparation. The commercial preparation of DMP 115 uses a mixture of DPPC, MPEG5000 DPPE, and DPPA to form the lipid shell (3). Immediately before use, the vial that contains the lipid mixture with a headspace of perflutren gas is agitated in a calibrated mechanical shaker for 45 s to produce a suspension of PFC bubbles (1.1-3.3 µm in size) within a lipid shell. If the preparation is not used within 5 min, the lipid microspheres must be resuspended by 10 s of hand agitation (inverting the vial).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Definity%20OR%20%22Perflutren%20Lipid%20Microsphere%22%29%20AND%20in%20vitro)]

Moran et al. (17) reported the in vitro acoustic characteristics of DMP 115 and 3 other US contrast agents in saline. The study found that, despite the different shell characteristics and gas compositions, these agents exhibited remarkably similar acoustic characteristics at 30 MHz. DMP 115 exhibited a peak mean backscatter power at concentrations between 1 х 10^6^ and 10 х 10^6^ microbubbles/ml. At concentrations lower than this, mean backscatter power decreased in a linear manner.

Sboros et al. (18) found that DMP 115 provided a constant number of scattering events per unit volume of suspension in water over acoustic pressures in the range of 0.2 to 1.5 MPa.

Toledo et al. (19) studied the feasibility of real-time three-dimensional echocardiography (RT3DE) with contrast enhancement in 9 isolated rabbit hearts. Administration of 1.3 ml DMP 115 in 25 ml of saline and infused at 16-25 ml/h showed clearly visible and uniform dynamic changes in myocardial video-intensity in all LV image slices at the 1.6-MHz transmit frequency (19).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Definity%20OR%20%22Perflutren%20Lipid%20Microsphere%22%29%20AND%20rodentia)]

Miller et al. (20) studied the potential cardiomyocyte injury induced by MCE in rats at high US mechanical index (MI) values greater than the recommended value of 0.8 for general clinical use. The study found that cardiomyocyte injury was not significant at 1.1-MPa end-systole triggering (MI = 0.9). At 1.6 and 2.0 MPa, the cardiomyocyte injury (indicated by Evans blue stain) showed a significant increase relative to the control cells. At 2.0 MPa, Evans blue-stained cell counts also increased with increasing MP 115 dose from 10 to 50 µl/kg.

Kobayashi et al. (21) investigated the influence of DMP 115 on microvessels in the rat mesentery and myocardium. The interaction between 0.1 ml/kg DMP 115 and US exposure did not cause microvessel bleeding and endothelial cell injury. When the dose was increased to 1.0 ml/kg, there was evidence of capillary bleeding and increased endothelial cell injury. Microvessel bleeding was not observed under any conditions.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Definity%20OR%20%22Perflutren%20Lipid%20Microsphere%22%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

Maruyama et al. (22) showed that DMP 115 could provide contrast enhancement of the VX-2 tumor in rabbit livers. Margins of the liver tumor were well-defined at DMP 115 doses of 10 µl/kg (MI = 0.6) and 30 µl/kg (MI = 0.2).

Toledo et al. (19) studied the RT3DE technology (MI = 0.4-0.8) with DMP 115 (1.3 ml in 25 ml of saline and infused at 150-260 ml/h) in 5 pigs with partial coronary occlusion. Administration of DMP 115 and RT3DE imaging showed that coronary occlusion caused a 59 ± 26% decrease in the calculated peak contrast inflow rate (PCIR) in agreement with measurements by fluorescent microspheres.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Definity%20OR%20%22Perflutren%20Lipid%20Microsphere%22%29%20AND%20%28primate%20NOT%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%28Definity%20OR%20%22Perflutren%20Lipid%20Microsphere%22%29%20AND%20human)]

Kitzman et al. (23) studied the efficacy and safety of DMP 115 in patients with suboptimal baseline LC echocardiographic images in a multicenter (17 sites), randomized, placebo-controlled, double-blind trial. Each patient received two i.v. doses of either 5 µl/kg (n = 85) or 10 µl/kg (n = 84) DMP 115 at 30 min apart. There was no clinically significant change in physical examination, vital signs, electrocardiographic tracings, or chemistry or hematology laboratory values. The adverse event rates were 18% compared with 14% in the placebo group (n = 42). Headache (5%) was the most frequent adverse event. Clinically useful contrast was recorded in 89% of patients compared with 0% of the placebo group. Improvement in endocardial border delineation was found in 91% of DMP 115 patients and in 12% of patients who received placebo.

Murthy et al. (10) investigated the real-time MCE (frame rates = 6-20 Hz; MI = 0.1-0.4) in 23 healthy volunteers. The DMP 115 doses ranged from 1,300 to 1,950 µl in 25-35 ml of normal saline and were given at an infusion rate of 4-6.5 ml/min. Real-time MCE appeared to give a more homogeneous opacification of the myocardium than that of triggered imaging. It was also possible to quantify flow reserve in normal healthy volunteers. Oraby et al. (24) used a newly developed US software, coherent contrast imaging (CCI), to perform real-time MCE in 42 men who had known or suspected coronary artery disease and adequate apical windows. They found that in this particular population of patients, it was feasible to use real-time CCI echocardiography to assess myocardial perfusion and LV wall motion. In 8 normal volunteers, Toledo et al. (19) used RT3DE imaging to show that adenosine increased PCIR to 198 ± 57% of baseline.

## Supplemental Information

[Disclaimers]

Perflutren package insert October 2007

## References

1 Benko L.B. (2004). UnitedHealth snags Definity. Mod Healthc.
2 Rosenberg M.L., Carpenter A.P. (2002). Contrast material-enhanced abdominal US examinations with DMP 115 (DEFINITY) provides additional diagnostic information with potential for changes in patient management. Acad Radiol.
3. Definity vial for (Perflutren Lipid Microsphere) injectable Suspension package insert. September 2004, Bristol-Myers Squibb Medical Imaging. p. 1-2.
4 Morawski A.M., Lanza G.A., Wickline S.A. (2005). Targeted contrast agents for magnetic resonance imaging and ultrasound. Curr Opin Biotechnol.
5 Schutt E.G., Klein D.H., Mattrey R.M., Riess J.G. (2003). Injectable microbubbles as contrast agents for diagnostic ultrasound imaging: the key role of perfluorochemicals. Angew Chem Int Ed Engl.
6. Swanson, D.P., Enhancement agents for ultrasound: Fundamentals, in Pharmaceuticals in Medical Imaging, D.P. Swanson, H.M. Chilton and J.H. Thrall, Editor. 1990, MacMillan Publishing Co., Inc.: New York. p. 682-687.
7. Gobuty, A.H., Perspectives in ultrasound contrast agents, in Contrast media: Biologic effects and clinical application, Z. Parvez, R. Moncada and M. Sovak, Editor. 1987, CRC: Boca Raton, Florida. p. 145-155.
8 Averkiou M., Powers J., Skyba D., Bruce M., Jensen S. (2003). Ultrasound contrast imaging research. Ultrasound Q.
9 Miller A.P., Nanda N.C. (2004). Contrast echocardiography: new agents. Ultrasound Med Biol.
10 Murthy T.H., Li P., Locvicchio E., Baisch C., Dairywala I., Armstrong W.F., Vannan M. (2001). Real-time myocardial blood flow imaging in normal human beings with the use of myocardial contrast echocardiography. J Am Soc Echocardiogr.
11 Riess J.G. (2001). Oxygen carriers ("blood substitutes")--raison d'etre, chemistry, and some physiology. Chem Rev.
12 Riess J.G. (2002). Blood substitutes and other potential biomedical applications of fluorinated colloids. Journal of Fluorine Chemistry.
13 Mattrey R.F., Trambert M.A., Brown J.J., Bruneton J.N., Young S.W., Schooley G.L. (1991). Results of the phase III trials with Imagent GI as an oral magnetic resonance contrast agent. Invest Radiol.
14 Pashkevich D.S., Shelopin G.G., Mukhortov D.A., Petrov V.B., Alekseev Y.I., Asovich V.S. (2004). and Synthesis of perfluoroalkanes by high-temperature reaction of graphite with fluorine in a fluidized bed. Macromolecular chemistry and polymeric materials, 77(11): p. 1847-1853.
15 Blomley M., Claudon M., Cosgrove D. (2007). WFUMB Safety Symposium on Ultrasound Contrast Agents: clinical applications and safety concerns. Ultrasound Med Biol.
16 Riess J.G. (2002). Fluorous micro- and nanophases with a biochemical perspective. Tetrahedron.
17 Moran C.M., Watson R.J., Fox K.A., McDicken W.N. (2002). In vitro acoustic characterisation of four intravenous ultrasonic contrast agents at 30 MHz. Ultrasound Med Biol.
18 Sboros V., Moran C.M., Pye S.D., McDicken W.N. (2003). The behaviour of individual contrast agent microbubbles. Ultrasound Med Biol.
19 Toledo E., Lang R.M., Collins K.A., Lammertin G., Williams U., Weinert L., Bolotin G., Coon P.D., Raman J., Jacobs L.D., Mor-Avi V. (2006). Imaging and quantification of myocardial perfusion using real-time three-dimensional echocardiography. J Am Coll Cardiol.
20 Miller D.L., Li P., Dou C., Gordon D., Edwards C.A., Armstrong W.F. (2005). Influence of contrast agent dose and ultrasound exposure on cardiomyocyte injury induced by myocardial contrast echocardiography in rats. Radiology.
21 Kobayashi N., Yasu T., Yamada S., Kudo N., Kuroki M., Miyatake K., Kawakami M., Saito M. (2003). Influence of contrast ultrasonography with perflutren lipid microspheres on microvessel injury. Circ J.
22 Maruyama H., Matsutani S., Saisho H., Kamiyama N., Yuki H., Miyata K. (2000). Grey-scale contrast enhancement in rabbit liver with DMP115 at different acoustic power levels. Ultrasound Med Biol.
23 Kitzman D.W., Goldman M.E., Gillam L.D., Cohen J.L., Aurigemma G.P., Gottdiener J.S. (2000). Efficacy and safety of the novel ultrasound contrast agent perflutren (definity) in patients with suboptimal baseline left ventricular echocardiographic images. Am J Cardiol.
24 Oraby M.A., Hays J., Maklady F.A., El-Hawary A.A., Yaneza L.O., Zabalgoitia M. (2002). Comparison of real-time coherent contrast imaging to dipyridamole thallium-201 single-photon emission computed tomography for assessment of myocardial perfusion and left ventricular wall motion. Am J Cardiol.